# BODIPY-FL-neutravidin-biotin-Cetuximab

Chemical name: | BODIPY-FL-neutravidin-biotin-Cetuximab
Abbreviated name: | BODIPY-FL-Cetuximab
Synonym:
Agent Category: | Antibody
Target: | HER1 receptor
Target Category: | Antibody binding to EGF receptor
Method of detection: | Optical fluorescence imaging
Source of signal: | BODIPY-FL
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=8815559), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=41327737) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=1956) for more information about EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cetuximab)]

Epidermal growth factor (EGF) is a cytokine (6.2 kDa) composed of 53 amino acids that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets (11-13). Target-specific optical activation has been studied on the basis of protease activation of quenched fluorophore-labeled enzyme substrates (14, 15). Another approach is based on the binding of biotin to BODIPY-FL–conjugated neutravidin (nAv) leading to an ~10-fold increase in fluorescence signal (16). The biotin-nAv binding inhibited the photon-induced electron transfer from aromatic amino acids to the excited state of BODIPY-FL, which led to dequenching of the BODIPY-FL. Cetuximab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER1 with an affinity constant of 0.1 nM. Cetuximab is available commercially in the United States and has been approved (http://www.cancer.gov/cancertopics/druginfo/cetuximab) by the U.S. Food and Drug Administration for the treatment of metastasized colorectal cancer and advanced squamous cell carcinoma of the head and neck. Cetuximab is currently being evaluated in several clinical trials (http://www.cancer.gov/search/ResultsClinicalTrialsAdvanced.aspx?protocolsearchid=2740900) for the treatment of a variety of cancers. Hama et al. (16) pretargeted peritoneal tumor metastases with biotin-cetuximab and then administered nAv-conjugated BODIPY-FL (nAv-BDPfl), which increased in fluorescence upon binding to biotin-cetuximab. BODIPY-FL is a green fluorescent dye with an absorbance maximum at 505 nm, an emission maximum at 513 nm, and a high extinction coefficient of 80,000 M^-1^cm^-1^.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BODIPY-FL-Cetuximab+and%20synthesis)]

Sulfosuccinimidyl-6-(biotin-amindo)hexanoate (120 nmol) was used to conjugate cetuximab (6.7 nmol) to form biotin-cetuximab (b-cetuximab), which was purified with gel-filtration chromatography (16). The molar ratio of biotin to cetuximab was estimated to be ~10. A single cetuximab molecule could be conjugated with 23 biotins (23b-cetuximab). Neutravidin (5.9 nmol) was incubated with 12 nmol BODIPY-FL-succinimidyl ester for 15 min at room temperature to form nAv-BDPfl, which was purified with gel-filtration chromatography. There were 1.3 BODIPY-FL molecules per neutravidin. Addition of nAv-BDPfl to b-cetuximab solution increased the fluorescence signal from 19.4 a.u. (cetuximab + nAv-BDPfl) to 173.1 a.u.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BODIPY-FL-Cetuximab%20and%20in%20vitro)]

Hama et al. (16) performed cell-binding assays with ^125^I-labeled b-cetuximab molecules using human epidermoid carcinoma A431 cells (overexpressing HER1). 12b-Cetuximab (72%) and 23b-cetuximab (68%) exhibited no loss of binding ability compared with unconjugated cetuximab (70%). Flow cytometry studies showed that 99.9% of A431 cells pretreated with b-cetuximab were positive after nAv-BDPfl addition, whereas only 1.1% of cells were positive with cetuximab pretreatment. The mean fluorescence intensity values were 6.8 a.u for cetuximab (plus nAv-BDPfl) and 680.0 a.u. for b-cetuximab (plus nAv-BDPfl), indicating activation of nAv-BDPfl upon binding to a biotinylated cetuximab antibody.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BODIPY-FL-Cetuximab%20and%20rodentia)]

Hama et al. (16) performed pretargeting studies in mice bearing A431 tumors in the peritoneal cavities using spectral fluorescence imaging. Biotinylated humanized control IgG_1_, cetuximab, b-cetuximab (0.7 nmol/mouse) were injected into the peritoneal cavity, followed by injection of nAv-BDPfl at 21 h. At 3 h after nAv-BDPfl injection, only tumors pretreated with b-cetuximab were clearly visualized, with little background fluorescence. For tumor foci (metastatic tumors and small tumor implants) of ≥0.8 mm in diameter, the spectral fluorescence imaging had a sensitivity of 96% (178 of 185 tumor foci) and a specificity of 98% (188 of 191 foci).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BODIPY-FL-Cetuximab%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BODIPY-FL-Cetuximab%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BODIPY-FL-Cetuximab%20and%20human)]

No relevant publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
12 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
13 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
14 Jaffer F.A., Libby P., Weissleder R. (2007). Molecular imaging of cardiovascular disease. Circulation.
15 Weissleder R., Tung C.H., Mahmood U., Bogdanov A. (1999). In vivo imaging of tumors with protease-activated near-infrared fluorescent probes. Nat Biotechnol.
16 Hama Y., Urano Y., Koyama Y., Choyke P.L., Kobayashi H. (2007). Activatable fluorescent molecular imaging of peritoneal metastases following pretargeting with a biotinylated monoclonal antibody. Cancer Res.